# Cyclic Arg-Gly-Asp-polyethyleneglycol-single-walled carbon nanotubes

Chemical name: | Cyclic Arg-Gly-Asp-polyethyleneglycol-single-walled carbon nanotubes
Abbreviated name: | RGD-PEG-SWNTs
Synonym: | RGD-SWNTs
Agent catgeory: | Peptide (nanoparticle)
Target: | Integrin α_υ_β_3_
Target category: | Receptor
Method of detection: | Optical imaging, Raman imaging, photoacoustic imaging
Source of signal/contrast: | Single-walled carbon nanotubes (SWNTs)
Activation: | No
Studies: | - Rodents | No structure is current available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD + SWNTs)]

The α_υ_β_3_ integrin, also known as the vitronectin receptor, is a heterodimeric transmembrane glycoprotein found on most cells originating from mesenchyme (1). This receptor is often overexpressed in various tumor cells, including osteosarcomas, neuroblastomas, glioblastomas, invasive melanomas, and carcinomas of the lung, breast, prostate, and bladder. Many extracellular matrix proteins such as fibronectin, vitronectin, thrombospondin, fibrinogen, osteopontin, and tenascin are known to be involved in interactions with various subtypes of integrins. These proteins may contain a variety of motifs for potential cell binding; however, one of the most frequent cell-recognition motifs includes an amino acid sequence of Arg-Gly-Asp (RGD), called the "universal cell-recognition site” or a "versatile cell recognition signal” (2). The binding potency of the RGD motif leads to the development of small homing peptides, whose high affinity to the α_υ_β_3_ integrin provides a promising alternative to antibodies in targeting tumors (3). As a result, RGD analogs are widely used in tumor imaging, anti-angiogenesis treatment, and tumor-associated radionucleotides or chemotherapeutic drugs. Some RGD analogs are currently being used in phase II clinical trials (4). These α_υ_β_3_ integrin–specific probes will help oncologists improve the delineation of tumors and follow up on the progression of anti-angiogenic therapies.

Single-walled carbon nanotubes (SWNTs) are composed of a single graphene sheet rolled into a tubular shape with a diameter of 0.4–2.0 nm and a length of 20–1,000 nm (5). Because of the graphene structure and seeming one-dimensionality, SWNTs exhibit unique thermal, physical, optical, and electrical properties (6). These properties are closely related to two integers (n, m), where n defines the length of the nanotube and m defines the chiral angle of rolling-up. For instance, SWNTs with the difference of n and m (n-m) evenly divisible by 3 belong to semiconductors and can generate a band gap–related fluorescence when suspended in solutions with surfactant micelles (7). The band gap of 1 eV corresponds to the “biological window” (700–1,300 nm) in fluorescence, where absorption, scattering, and autofluorescence by tissues, blood, and water are at a minimum (8). These optical properties make SWNTs appealing as a contrast agent for near-infrared (NIR) bioluminescence imaging and as an optical absorption agent (8) for photoacoustic imaging (9). In photoacoustic imaging, short pulses of stimulating radiation are absorbed by chromophores in tissues, resulting a subsequent thermal expansion and ultrasonic emission that can be detected by highly sensitive piezoelectric devices (10). Photoacoustic imaging as an emerging modality combines the high optical absorption contrast with diffraction-limited resolution of ultrasonic imaging. In addition, the inherent structure of graphene makes SWNTs an excellent contrast agent for Raman imaging (11). The tangential vibrations in the nanotubes generate diameter-selective resonance Raman scattering that is characterized by a major Raman peak located at the G-band (~1,590 cm^-1^). SWNTs prepared by various methodologies are hydrophobic. The SWNT surface can be modified with surfactants to increase solubility in aqueous solutions or functionalized with bioactive ligands to target specific sites in tissues (12). Cyclic RGD-polyethyleneglycol-SWNTs (RGD-PEG-SWNTs) are functionalized SWNTs used for Raman imaging (11) or photoacoustic imaging (9) of α_υ_β_3_ integrin.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(RGD + SWNTs)+AND+synthesis%0D%0A)]

Liu et al. briefly described the synthesis of RGD-SWNTs (13). Initially, SWNTs were prepared with the use of raw gas-phase decomposition of high-pressure carbon monoxide (HiPCO). The obtained SWNTs were sonicated in an aqueous solution of 1,2-distearoyl-sn-glycero-3-phosphoethanolamine-N-(amine(polyethyleneglycol)_2000_) (DSPE-PEG_2000_-NH_2_) or 1,2-distearoyl-sn-glycero-3-phosphoethanolamine-N-(amine(polyethyleneglycol)_5400_) (DSPE-PEG_5400_-NH_2_) for 1 h followed by centrifugation at 24,000 g for 6 h to functionalize SWNTs. The produced SWNT-PEG-NH_2_ was further conjugated with sulphosuccinimidyl 4-N-maleimidomethyl cyclohexane-1-carboxylateat (sulpho-SMCC) (pH 7.2) for 2 h then reacted with thiolated RGD (pH 7.4) overnight, yielding RGD-PEG_2000_-SWNTs or RGD-PEG_5400_-SWNTs.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(RGD + SWNTs)+AND+%22in+vitro%22)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(RGD + SWNTs) +AND++rodentia)]

Liu et al. used ex vivo biodistribution and in vivo positron emission tomography (PET) to examine the biodistribution of RGD-PEG_5400_-SWNTs via ^64^Cu labeling (13). In both studies, nude mice bearing U87MG tumors received injections of ~200–300 mCi ^64^Cu-labeled RGD-PEG_5400_-SWNTs. For the ex vivo measurement of biodistribution, the mice were euthanized 24 h post-injection (p.i.), and the tissues were harvested for γ-counting. The tumor uptake increased rapidly, reached a plateau at 6 h p.i., and leveled off in the next 20 h. The measured radioactivity in tumors was 10–15% injected dose (ID)/g for RGD-PEG_5400_-SWNTs, compared to the 3–4% for PEG_5400_-SWNTs. The uptake in other tissues was found to be ~20% ID/g in liver, ~8% ID/g in kidney, and <2% ID/g in blood. As a control, 15 mg/kg c(RGDyK) was co-administrated as a block agent with ^64^Cu-labeled RGD-PEG_5400_-SWNTs, which significantly reduced the tumor uptake of RGD-PEG_5400_-SWNTs. In addition, mice bearing integrin α_υ_β_3_–negative tumors (HT-29) were injected with ^64^Cu-labeled RGD-PEG_5400_-SWNTs. No apparent tumor uptake was found. Liu et al. also examined the biodistribution of RGD-PEG_2000_-SWNTs using the same approach (13). Compared to ^64^Cu-labeled RGD-PEG_5400_-SWNTs, RGD-PEG_2000_-SWNTs exhibited a lower uptake in U86MG tumors (~5% ID/g) and a higher uptake in the liver (~30% ID/g). To confirm the results, mice bearing U87MG tumors were injected with a high dose of RGD-PEG_5400_-SWNTs (0.5 mg/kg) and euthanized 8 h p.i. The tumoral and liver tissues were excised for Raman spectroscopic measurement. A high intensity at the G-band (~1,580 cm^-1^) was found in these tissues, validating the presence of SWNTs. These results demonstrated that the uptake occurred via the reticuloendothelial system (RES), very similar to uptake of nanoparticles 10–100 nm in diameter.

Keren et al. used RGD-PEG-SWNTs to obtain in vivo Raman imaging (11). Mice bearing U87MG tumors were injected intravenously with a 200-μl solution containing 60 pmol RGD-PEG-SWNTs. Raman images were collected 24 h p.i. at 1,593 cm^-1^. A strong Raman signal was found in the tumoral area. As a control, mice bearing U87MG tumors were intravenously injected with PEG-SWNTs and examined at the same imaging conditions. No apparent accumulation was found in the tumor area. De la Zerda et al. used RGD-PEG-SWNTs to obtain in vivo photoacoustic imaging (9). Mice (n = 4) bearing U87MG tumors (~100 mm^3^) were injected intravenously with a 200-μl solution at a concentration of 1.2 μM RGD-PEG-SWNTs. Three-dimensional ultrasound and photoacoustic images were collected for the tumors and their surrounding tissues before injection and up to 4 h p.i. A consistent increase in the photoacoustic signal of the tumor was observed. In comparison, the signal increase as a result of PEG-SWNTs was transient. The accumulation of RGD-PEG-SWNTs in the tumors was found three to five times higher than that of PEG-SWNTs, yielding an approximately eight-fold increase in photoacoustic signal.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(RGD + SWNTs) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(RGD + SWNTs) +AND+human)]

No publication is currently available.

### NIH Support

CA 119367, EB000312, CA 114747, CA 09695

## References

1 Haubner R., Finsinger D., Kessler H. (1997). Stereoisomeric peptide libaries and peptidomimetics for designing selective inhibitors of the a_υ_β_3_ integrin for a new cancer therapy. Angew. Chem. Int. Ed. Engl.
2 Ruoslahti E., Pierschbacher M.D. (1986). Arg-Gly-Asp: a versatile cell recognition signal. Cell.
3 Zitzmann S., Ehemann V., Schwab M. (2002). Arginine-glycine-aspartic acid (RGD)-peptide binds to both tumor and tumor-endothelial cells in vivo. Cancer Res.
4 Garanger E., Boturyn D., Dumy P. (2007). Tumor targeting with RGD peptide ligands-design of new molecular conjugates for imaging and therapy of cancers. Anticancer Agents Med Chem.
5 Lacerda L., Bianco A., Prato M., Kostarelos K. (2006). Carbon nanotubes as nanomedicines: from toxicology to pharmacology. Adv Drug Deliv Rev.
6 Welsher K., Liu Z., Daranciang D., Dai H. (2008). Selective probing and imaging of cells with single walled carbon nanotubes as near-infrared fluorescent molecules. Nano Lett.
7 Bachilo S.M., Strano M.S., Kittrell C., Hauge R.H., Smalley R.E., Weisman R.B. (2002). Structure-assigned optical spectra of single-walled carbon nanotubes. Science.
8 Choi J.H., Nguyen F.T., Barone P.W., Heller D.A., Moll A.E., Patel D., Boppart S.A., Strano M.S. (2007). Multimodal biomedical imaging with asymmetric single-walled carbon nanotube/iron oxide nanoparticle complexes. Nano Lett.
9 De la Zerda A., Zavaleta C., Keren S., Vaithilingam S., Bodapati S., Liu Z., Levi J., Smith B.R., Ma T.J., Oralkan O., Cheng Z., Chen X., Dai H., Khuri-Yakub B.T., Gambhir S.S. (2008). Carbon nanotubes as photoacoustic molecular imaging agents in living mice. Nat Nanotechnol.
10 Wang L., Xie X., Oh J.T., Li M.L., Ku G., Ke S., Similache S., Li C., Stoica G. (2005). Combined photoacoustic and molecular fluorescence imaging in vivo. Conf Proc IEEE Eng Med Biol Soc.
11 Keren S., Zavaleta C., Cheng Z., de la Zerda A., Gheysens O., Gambhir S.S. (2008). Noninvasive molecular imaging of small living subjects using Raman spectroscopy. Proc Natl Acad Sci U S A.
12 Prato M., Kostarelos K., Bianco A. (2008). Functionalized carbon nanotubes in drug design and discovery. Acc Chem Res.
13 Liu Z., Cai W., He L., Nakayama N., Chen K., Sun X., Chen X., Dai H. (2007). In vivo biodistribution and highly efficient tumour targeting of carbon nanotubes in mice. Nat Nanotechnol.